# ^64^Cu-Labeled cysteine–tagged dimeric epidermal growth factor

Chemical name: | ^64^Cu-Labeled cysteine–tagged dimeric epidermal growth factor
Abbreviated name: | [^64^Cu]Cys-dEGF; dEGF-PEG-DOTA/Cu
Synonym:
Agent Category: | Ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide sequence (http://www.ncbi.nlm.nih.gov/nuccore/166362727?report=genbank) of human epidermal growth factor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=role+of+growth+factors+in+cancer)]

Growth factors such as the epidermal growth factor (EGF), the vascular endothelial growth factor (VEGF), and the tumor necrosis factor are known to have important roles in the development and progression of cancers (1-3). The EGF mediates its activity through a group of tyrosine kinase (TK)–dependent EGF receptors (EGFR) that promote not only cell proliferation but also cell survival and the motility phenotype that is necessary for the development of an invasive cancer (4). As a consequence, the EGFRs and their associated TKs are the targets of several anti-EGFR antibodies (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies) and TK inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors) that are either approved by the United Stated Food and Drug Administration or are being evaluated in clinical trials for the treatment of various neoplasms. Before treatment, the patients are screened to determine the extent of EGFR expression in the tumors with the use of immunohistochemistry (IHC) or fluorescence in situ hybridization (FISH) because these techniques help predict the probable therapeutic response and outcome for the individual (5, 6). However, only 10–25% of the patients who are EGFR-positive according to IHC or FISH analysis respond to the anti-EGFR therapy, which indicates that a poor correlation exists between the EGFR expression analysis and the treatment (7, 8). This is probably because only the active receptors are important to predict efficacy of the anti-EGFR agents for the treatment of cancers, and ICH and FISH do not distinguish between the active and inactive EGFRs (9).

On binding the ligand, a characteristic feature of a functional EGFR is that it is internalized by the cell. Levashova et al. (10) envisioned that perhaps the natural ligand EGF itself could be used as an imaging agent to detect the active EGFRs in tumors. The investigators used an Escherichia coli (E. coli)–expressed EGF containing an N-terminal cysteine fusion tag (Cys-EGF) of 15 amino acids that can be used to conjugate therapeutic or imaging probes as done earlier with VEGF (11). In addition, because an active EGF/EGFR complex is composed of two molecules each of EGF and EGFR, the investigators also bioengineered an N-terminal cysteine fusion tag containing a dimeric EGF (dEGF) molecule, with the second EGF molecule linked to the first through a linker of 9 amino acids (11). The EGF and the dEGF were then labeled with radioactive copper (^64^Cu) to obtain [^64^Cu]Cys-EGF and [^64^Cu]Cys-dEGF. The biodistribution and imaging characteristics of the two molecules were then investigated in mice bearing xenograft tumors. It is pertinent to mention here that the imaging and biodistribution studies of only [^64^Cu]Cys-dEGF are described in this chapter. Investigations performed with [^64^Cu]Cys-EGF are described separately in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cys-tagged+EGF+synthesis)]

The Cys-dEGF was expressed in and purified from E. coli as described elsewhere to obtain Cys-tagged single-chain VEGF (Cys-scVEGF) (12). Purified Cys-EGF was labeled with ^64^Cu as described elsewhere (12) with a procedure developed to label scVEGF using pegylated-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (PEG-DOTA). The dEGF-PEG-DOTA complex was purified with reverse-phase high-performance liquid chromatography, and purity of the product was reported to be >90% (10). Unconjugated ^64^Cu was removed by the addition of ethylenediamine tetraacetic acid, and the radiolabeled Cys-dEGF (dEGF-PEG-DOTA/Cu) was purified with size-exclusion chromatography on a NP-5 column (10). The radiochemical purity of dEGF-PEG-DOTA/Cu was not reported. Specific activity of dEGF-PEG-DOTA/Cu was reported to be ~2.7 MBq/μg (~75 μCi/μg) (10). The stability of dEGF-PEG-DOTA/Cu was reported to be at least 3 h at room temperature in phosphate-buffered saline and at least 75 min at 37°C in plasma (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Cys-EGF+in+vitro)]

The EGFR affinity constant for dEGF-PEG-DOTA/Cu was not reported (10); however, dEGF-PEG-DOTA was reported to induce EGFR TK phosphorylation in F98/EGFR cells in a dose-dependent manner (10). In another study, dEGF-PEG-DOTA/Cu was reported to compete with an EGF-Shiga-like toxin subunit A conjugate (EGF-SLT (http://www.sibtech.com/?p=targeted_toxins)) for binding to the EGFR (10). EGF-SLT is extremely toxic to MDA23 1luc human breast cancer cells, and the ability of proteins to compete for binding with the EGFR was measured by counting the number of cells surviving after a 72-h exposure to EGF-SLT (1 nM) in the presence of an increasing concentration of Cys-dEGF (0–25 nM). It was reported that cell survival increased with an increasing dEGF-PEG-DOTA/Cu concentration under these experimental conditions, which indicates that dEGF-PEG-DOTA/Cu protected the cells from EGF-SLT toxicity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+rodentia)]

Levashova et al. studied the blood clearance and biodistribution of dEGF-PEG-DOTA/Cu in mice (n = 4 animals) bearing F98/EGFR or MDA23 1luc cell tumors (10). The animals were injected with the radiotracer, and blood was collected at preselected time points for up to 60 min. More than 95% of the radioactivity was reported to clear from blood within 60 min. To determine biodistribution of the labeled protein, the animals were euthanized 3 h after administration of the tracer, all the major organs and tumors were harvested, and incorporated radioactivity in the harvested organs was counted using a gamma counter. The radioactivity was reported to have accumulated primarily in the liver and kidneys (~3.25% injected dose/gram tissue in both organs). Also, the MDA23 1luc cell tumors were reported to have a higher accumulation of radioactivity than the F98/EGFR cell tumors, although the former cells are known to express approximately five-fold less EGFR compared with the latter cells (10). The investigators suggested that this was probably because a higher number of functional receptors were present in the MDA23 1luc cells than in the F98/EGFR cells. No competition studies were reported. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Wu W.K., Tse T.T., Sung J.J., Li Z.J., Yu L., Cho C.H. (2009). Expression of ErbB receptors and their cognate ligands in gastric and colon cancer cell lines. Anticancer Res.
2 Schoenleber S.J., Kurtz D.M., Talwalkar J.A., Roberts L.R., Gores G.J. (2009). Prognostic role of vascular endothelial growth factor in hepatocellular carcinoma: systematic review and meta-analysis. Br J Cancer.
3 Balkwill F. (2009). Tumour necrosis factor and cancer. Nat Rev Cancer.
4 Wilkins-Port C.E., Ye Q., Mazurkiewicz J.E., Higgins P.J. (2009). TGF-beta1 + EGF-initiated invasive potential in transformed human keratinocytes is coupled to a plasmin/MMP-10/MMP-1-dependent collagen remodeling axis: role for PAI-1. Cancer Res.
5 Baselga J., Arteaga C.L. (2005). Critical update and emerging trends in epidermal growth factor receptor targeting in cancer. J Clin Oncol.
6 Varella-Garcia M., Mitsudomi T., Yatabe Y., Kosaka T., Nakajima E., Xavier A.C., Skokan M., Zeng C., Franklin W.A., Bunn P.A., Hirsch F.R. (2009). EGFR and HER2 genomic gain in recurrent non-small cell lung cancer after surgery: impact on outcome to treatment with gefitinib and association with EGFR and KRAS mutations in a Japanese cohort. J Thorac Oncol.
7 Chung K.Y., Shia J., Kemeny N.E., Shah M., Schwartz G.K., Tse A., Hamilton A., Pan D., Schrag D., Schwartz L., Klimstra D.S., Fridman D., Kelsen D.P., Saltz L.B. (2005). Cetuximab shows activity in colorectal cancer patients with tumors that do not express the epidermal growth factor receptor by immunohistochemistry. J Clin Oncol.
8 Bell D.W., Lynch T.J., Haserlat S.M., Harris P.L., Okimoto R.A., Brannigan B.W., Sgroi D.C., Muir B., Riemenschneider M.J., Iacona R.B., Krebs A.D., Johnson D.H., Giaccone G., Herbst R.S., Manegold C., Fukuoka M., Kris M.G., Baselga J., Ochs J.S., Haber D.A. (2005). Epidermal growth factor receptor mutations and gene amplification in non-small-cell lung cancer: molecular analysis of the IDEAL/INTACT gefitinib trials. J Clin Oncol.
9 Johns T.G., Perera R.M., Vernes S.C., Vitali A.A., Cao D.X., Cavenee W.K., Scott A.M., Furnari F.B. (2007). The efficacy of epidermal growth factor receptor-specific antibodies against glioma xenografts is influenced by receptor levels, activation status, and heterodimerization. Clin Cancer Res.
10 Levashova Z., Backer M.V., Horng G., Felsher D., Backer J.M., Blankenberg F.G. (2009). SPECT and PET imaging of EGF receptors with site-specifically labeled EGF and dimeric EGF. Bioconjug Chem.
11 Levashova Z., Backer M., Backer J.M., Blankenberg F.G. (2008). Direct site-specific labeling of the Cys-tag moiety in scVEGF with technetium 99m. Bioconjug Chem.
12 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.